# About MICAD

The Molecular Imaging and Contrast Agent Database (MICAD) is an online source of scientific information regarding molecular imaging and contrast agents (under development, in clinical trials or commercially available for medical applications) that have in vivo data (animal or human) published in peer-reviewed scientific journals. MICAD is a key component of the “Molecular Libraries and Imaging” program of the National Institutes of Health (NIH) Common Fund (formerly NIH Roadmap), that encompasses a set of major inter-agency initiatives designed to accelerate medical research for disease detection, diagnosis and therapy. By linking programs in molecular imaging, molecular probes, and molecular libraries, the NIH Common Fund provides much needed support for the development of new, more specific therapies for a wide range of diseases such as cancers, Alzheimer’s and Parkinson's diseases. MICAD is edited by a team of scientific editors and curators who are based at the National Library of Medicine, NIH, in Bethesda, Maryland. This program is under the guidance of a trans-NIH panel of experts in the field.

The database includes, but is not limited to, agents developed for positron emission tomography (PET), single photon emission computed tomography (SPECT), magnetic resonance imaging (MRI), ultrasound (US), computed tomography (CT), optical imaging, planar radiography, and planar gamma imaging. The information on each agent is summarized in a book chapter format containing several sections such as Background, Synthesis, in vitro studies, Animal Studies (with sub-sections: rodents, other non-human primate animals, and human primates), Human Studies, and References. In addition, the references are linked to PubMed for retrieval of the publication abstract. Also, each chapter contains links to resources at the National Center for Biotechnology Information (NCBI) and other relevant databases regarding the target of the imaging probe or contrast agent.

NIH Members
Christopher Austin, NHGRI Robert Balaban, NHLBI Linda Brady, NIMH Martin Brechbiel, NCI Steve Bryant, NLM Denis Buxton, NHLBI Arvind Chopra, NLM Jamie Driscoll, NIMH | Steven Grant, NIDA John Haller, NIBIB John Hoffman, NCI Michael Huerta, NIMH Robert Innis, NIMH Peter Kirchner, NIBIB Kam Leung, NLM David Lipman, NLM | Peter Lyster, NIGMS Anne Menkens, NCI Marc Nicklaus, NCI Victor Pike, NMIH Belinda Seto, NIBIB Liang Shan, NLM Terry Yoo, NLM

Extramural Members
William C. Eckelman – Molecular Tracer, LLC Richard Frank - GE Healthcare Sam Gambhir – Stanford Robert Mach - Washington U Tom Meade – Northwestern | Claude Meares - UC Davis Adrian Nunn – Bracco Brian Roth – Case Western Dean Sherry - UT Dallas Daniel Sullivan - Duke | Jean-Luc Vanderheyden – GE Healthcare Doug Wagenaar – Gamma Medica-Ideas Ralph Weissleder - Harvard Sam Wickline – Washington U